# (R,S)-2-(N-Propyl-N-5'-[^18^F]fluoropentyl)amino-5-hydroxytetralin

Chemical name: | (R,S)-2-(N-Propyl-N-5'-[^18^F]fluoropentyl)amino-5-hydroxytetralin
Abbreviated name: | [^18^F]-5-OH-FPPAT
Synonym: | (R,S)-5-Hydroxy-2-(N-propyl-N-(5'-[^18^F]fluoropentyl)aminotetralin
Agent Category: | Compound
Target: | D_2_ and D_3_ dopamine receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-5-OH-FPPAT)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five dopamine receptor subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_). D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system levels. Most striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons.

Dopamine receptors are G-protein–coupled receptors and exist in high- and low-affinity states with respect to agonist binding. The two states are interconvertible. In the high-affinity state, dopamine receptors are coupled to G-proteins, whereas in the low-affinity state they are not. Dopamine has a dissociation constant (K_d_) of 7 nM for the high-affinity state (K_high_) and a K_d_ of 1,720 nM for the low-affinity state (K_low_) (5). Under physiologic conditions, dopamine is expected to bind predominately to receptors in the high-affinity state. The high-affinity state was suggested to be the functional form of the dopamine receptors (6).

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2/3_ receptors, making studies of extrastriatal D_2/3_ receptors difficult (7-9). In binding studies, [^123^I]epidepride was found to have high potency and low nonspecific binding, and to be selective for striatal and extrastriatal D_2/3_ receptors (10). Epidepride exhibits marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective, high-affinity antagonist of D_2/3_ receptors (11), and in positron emission tomography (PET) in vivo studies (12-15) it identified extrastriatal D_2/3_ receptors. However, none of these antagonists distinguishes between the high- and low-affinity states of the D_2_ receptors. Many effects have been pursued to develop radiolabeled agonists for the non-invasive study of the high-affinity state of the D_2/3_ receptors in the brain. (–)-N-[^11^C]Propyl-norapomorphine ([^11^C]NPA) and [^11^C](+)-4-N-propyl-,3,4a,5,6,10b-hexahydro-2H-naphth[1,2-b][1,4]oxazin-9-ol ([^11^C]PHNO) have been studied as radiolabeled dopamine agonists.

Various hydroxytetralin analogs with different binding affinities for the D_2_ receptors have been developed as ^11^C-labeled agonist radiotracers (16). (R,S)-2-(N-propyl-N-5'-[^18^F]fluoropentyl)amino-5-hydroxytetralin ([^18^F]-5-OH-FPPAT) is being evaluated as a PET agent for the high-affinity state of D_2/3_ receptors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-5-OH-FPPAT%20and%20synthesis)]

Shi et al. (17) reported a three-step synthesis of [^18^F]-5-OH-FPPAT. 2-(N-propyl-N-5'-bromovaleryl)amino-5-tetrahydropyranyltetralin was reacted first with [^18^F]KF/Kryptofix 2.2.2, followed by LiAlH_4_ reduction and acidic deprotection, with a radiochemical yield of 10–15% (decay-corrected) at the end of bombardment and an average specific activity of 56–74 GBq/μmol (1.5–2.0 Ci/μmol) at end of synthesis after purification by high-performance liquid chromatography.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-5-OH-FPPAT%20and%20in%20vitro)]

In a binding study of dopamine receptors in membranes of the rat striata with [^18^F]fallypride, 5-OH-FPPAT had an inhibitory concentration (IC_50_) of 6.95 nM (17). In vitro autoradiography studies of rat brain slices indicated selective binding of [^18^F]-5-OH-FPPAT to the striata, which was almost completely inhibited by co-incubation with 10 μM sulpiride (a D_2/3_ antagonist) and Gpp(NH)p (conversion of the high-affinity states to the low-affinity states). There was little specific binding in the cortex and cerebellum, with a striata/cerebellum ratio of 17.4, a striata/cortex ratio of 12.8, and a cortex/cerebellum ratio of 1.35.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-5-OH-FPPAT%20and%20rodentia)]

Biodistribution studies in rats showed a marked accumulation of the tracer in the striata with 1.65% injected dose per gram (%ID/g) at 15 min after injection of [^18^F]-5-OH-FPPAT (17). The striata/cerebellum ratio was 1.9 at 30 min and 2.0 at 60 min. Significant nonspecific binding was observed in the cortical regions and cerebellum. The cortex/cerebellum ratio was 1.28 at 30 min and 1.35 at 60 min. Pretreatment with risperidone (0.05 mg/kg) and PPHT (0.1 mg/kg), both D_2/3_ antagonists, reduced specific binding of [^18^F]-5-OH-FPPAT to the striata by 40%. [^18^F]-5-OH-FPPAT showed higher striata/cerebellum ratio than the ^11^C-labeled hydroxytetralin analogs, such as [^11^C]PPHT and [^11^C]ZYY-339. Uptake of [^18^F]-5-OH-FPPAT is comparable to [^11^C]-5-OH-DPAT.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-5-OH-FPPAT%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-5-OH-FPPAT%20and%20monkey)]

Shi et al. (17) showed uptake in the brain (0.05% ID/ml) of rhesus monkeys with striata/cerebellum ratios of 1.5 at 10 min and 2.0 at 40 min after injection of 111 MBq (3 mCi) of [^18^F]-5-OH-FPPAT. The thalamus/cerebellum ratio was 1.4 at 40 min. The striata showed slower clearance than the cortex and cerebellum. The authors suggested that use of the more active S-isomer may provide a higher striata/cerebellum and thalamus/cerebellum ratios. [^18^F]-5-OH-FPPAT showed higher striata/cerebellum ratios than ^11^C-labeled hydroxytetralin analogs, such as [^11^C]PPHT and [^11^C]ZYY-339.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-5-OH-FPPAT%20and%20human)]

No publication is currently available.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Sunahara R.K., Guan H.C., O'Dowd B.F., Seeman P., Laurier L.G., Ng G., George S.R., Torchia J., Van Tol H.H., Niznik H.B. (1991). Cloning of the gene for a human dopamine D5 receptor with higher affinity for dopamine than D1. Nature.
6 Sibley D.R., De Lean A., Creese I. (1982). Anterior pituitary dopamine receptors. Demonstration of interconvertible high and low affinity states of the D-2 dopamine receptor. J Biol Chem.
7 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
8 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
9 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
10 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
11 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
12 Grunder G., Landvogt C., Vernaleken I., Buchholz H.G., Ondracek J., Siessmeier T., Hartter S., Schreckenberger M., Stoeter P., Hiemke C., Rosch F., Wong D.F., Bartenstein P. (2006). The striatal and extrastriatal d2/d3 receptor-binding profile of clozapine in patients with schizophrenia. Neuropsychopharmacology.
13 Kessler R.M., Ansari M.S., Riccardi P., Li R., Jayathilake K., Dawant B., Meltzer H.Y. (2005). Occupancy of striatal and extrastriatal dopamine d(2)/d(3) receptors by olanzapine and haloperidol. Neuropsychopharmacology.
14 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
15 Riccardi P., Li R., Ansari M.S., Zald D., Park S., Dawant B., Anderson S., Doop M., Woodward N., Schoenberg E., Schmidt D., Baldwin R., Kessler R. (2006). Amphetamine-induced displacement of [(18)f] fallypride in striatum and extrastriatal regions in humans. Neuropsychopharmacology.
16 Shi B., Narayanan T.K., Yang Z.Y., Christian B.T., Mukherjee J. (1999). Radiosynthesis and in vitro evaluation of 2-(N-alkyl-N-1'-11C-propyl)amino-5-hydroxytetralin analogs as high affinity agonists for dopamine D-2 receptors. Nucl Med Biol.
17 Shi B., Narayanan T.K., Christian B.T., Chattopadhyay S., Mukherjee J. (2004). Synthesis and biological evaluation of the binding of dopamine D2/D3 receptor agonist, (R,S)-5-hydroxy-2-(N-propyl-N-(5'-(18)F-fluoropentyl)aminotetralin ((18)F-5-OH-FPPAT) in rodents and nonhuman primates. Nucl Med Biol.